# ^99m^Tc^(v)^O-Gly-Gly-Cys-Orn-Orn-Orn-Bombesin[2-14]

Chemical name: | ^99m^Tc^(v)^O-Gly-Gly-Cys-Orn-Orn-Orn-Bombesin[2-14] | [image]
Abbreviated name: | ^99m^Tc-N_3_S-X-BN[2-14] | [image]
Synonym: | ^99m^Tc-N_3_S-Orn-Orn-Orn-BN[2-14], ^99m^Tc-N_3_S-BN[2-14] | [image]
Agent Category: | peptide | [image]
Target: | Gastrin-releasing peptide receptor (GRPR) | [image]
Target Category: | Receptor | [image]
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging | [image]
Source of signal / contrast: | ^99m^Tc | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of N_3_S-X-BN[2-14], where X=Orn-Orn-Orn. Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=4885361), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=61677286) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2925) for more information about gastrin-releasing peptide receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22bombesin%22%25GRPR%20imaging)]

^99m^Tc^(v)^O-Gly-Gly-Cys-Orn-Orn-Orn-Bombesin[2-14] (^99m^Tc-N_3_S-X-BN[2-14]) is a bombesin (BN) derivative synthesized and labeled with ^99m^Tc by Fragogeorgi et al. for molecular imaging of tumors expressing gastrin-releasing peptide receptor (GRPR) (1).

BN is an amphibian neuropeptide consisting of 14 amino acids (pGlu-Gln-Arg-Leu-Gly-Asn-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_) (2, 3), and it was first isolated from frog skin in 1970 (4). The search for its mammalian counterpart led to the discovery of gastrin-releasing peptide (GRP), which consists of 27 amino acids. GRP and BN share an identical C-terminal region (-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_), which is necessary for receptor binding and signal transduction (5, 6). In addition to the release of gastrin, GRP- and BN-like peptides also produce a wide range of other biological responses in diverse tissues, such as secretion of endocrine and exocrine glands, maintenance of circadian rhythm, regulation of satiety, and contraction of smooth muscles (7). They also act as potential growth factors for both normal and cancerous cells (3, 5, 6). There are four members of the BN receptor family, including three mammalian receptors: GRPR (BB_2_ or BRS2; 384 amino acids), neuromedin B receptor (NMBR, BB_1_, or BRS1; 390 amino acids), and BN-like receptor 3 (BB_3_, BRS3, or orphan; 399 amino acids) (5, 7, 8); the fourth receptor (BB_4_) has only been found in amphibians. GRPR is the only well characterized receptor of this family. GRPR is a glycosylated, 7-transmembrane, G-protein–coupled receptor that, upon binding with its ligands, gives rise to a complex cascade of intracellular reactions. It is normally found in non-neuroendocrine tissues of the breast and pancreas, and in neuroendocrine cells of the brain, gastrointestinal tract, lung, and prostate (9). Interestingly, GRPR is overexpressed in prostate cancer as well as in tumors of the breast, lung, pancreas, ovary, kidney, and gastrointestinal tract. It has been reported that GRPR is expressed at a high density in the intraepithelial neoplasia and primary carcinoma of the prostate, whereas normal prostate tissue and, in most cases, benign prostate hyperplasia are predominantly negative for GRPR (10-13).

GRPR has attracted significant interest as a target for tumor detection, tumor staging, and evaluation of tumor response to therapy (5, 6, 8, 11). A large number of BN derivatives have been developed, and they have been labeled with ^99m^Tc, ^177^Lu, ^67^Ga, and ^111^In for single-photon emission computed tomography (SPECT) and with ^64^Cu, ^68^Ga, and ^18^F for positron emission tomography. The published BN derivatives can be generally classified as truncated BN (6–14 or 7–14) or full-length BN (1-14) analogs (10, 12-18). The truncated BN analogs seem to be favorable for in vivo applications because they are usually more stable than the full-length tetradecapeptides and still bind to the GRPR adequately. However, the full-length peptides offer different labeling methods by attachment of functional groups to the amino acids 1–6. In many cases, the amino acids on positions 13 (Leu) and 14 (Met) have been replaced by unnatural amino acids (cyclohexylalanine (CyHAla) and norleucine (Nle)), and Lys has been placed on position 3 for attachment of radiolabels with reactive esters. Spacers, chelators, or radiometals have also been widely used for conjugation and for favorable kinetics (1). The BN derivatives can also be divided into agonists and antagonists (19-21). By far, most BN derivatives are agonists. Agonists are internalized into and accumulate within cells, and it has been assumed that they exhibit higher uptake by cancer cells than antagonists. However, some reports have shown that uptake of antagonists in vivo into tumor xenografts is higher than that of agonists (19, 20). Antagonists may have stronger binding for the GRPR than agonists (19, 20). It has been suggested that antagonists may bind to all of the receptors whereas agonists may only bind to the high affinity sites of the receptors.

An optimal BN-like radiotracer needs to meet several requirements: high affinity for GRPR, with rapid and specific tumor uptake; high hydrophilicity, with preferred renal excretion and low hepatobiliary excretion; and high stability but relatively rapid clearance from blood (6). Despite a large number of published derivatives, a valid comparison among them for the feasibility of tumor imaging is difficult because standardization between studies is lacking. Generally speaking, the majority of the radiotracers have relatively high renal and hepatic uptake, resulting in low tumor/liver and tumor/kidney ratios. In an effort to improve the binding property and optimize the biodistribution, Fragogeorgi et al. developed two ^99m^Tc-labeled BN derivatives with different hydrophilicities and overall charges (1). One BN derivative had a sequence of ^99m^Tc^(v)^O-Gly-Gly-Cys-bombesin[2-14] (^99m^Tc-N_3_S-BN[2-14]). Another BN derivative had the same sequence, but a basic amino acid spacer (Orn-Orn-Orn) was introduced (^99m^Tc-N_3_S-X-BN[2-14], where X = Orn-Orn-Orn), and this BN derivative was more hydrophilic than ^99m^Tc-N_3_S-BN[2-14]. Comparative studies between the two BN derivatives showed that hydrophilicity and charge strongly affected their binding properties and biodistribution patterns. ^99m^Tc-N_3_S-X-BN[2-14] was superior to ^99m^Tc-N_3_S-BN[2-14] for use in SPECT imaging of tumors (1).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=(99m)Tc-N(3)S-X-Bombesin)]

Both BN derivatives were prepared by Fragogeorgi et al. with the solid-phase peptide synthesis technique (1). Briefly, an excess of fluorenylmethoxycarbonyl (Fmoc)-protected amino acids and N-hydroxybenzotriazole were dissolved in N,N’-dimethylformamide (DMF). The solution was cooled in ice, and N,N’-diisopropylcarbodiimide was then added to the solution. The reaction mixture was initially left for 10 min on ice, and then for 10 min at room temperature, before being added to the resin. Removal of the N-terminal Fmoc group was achieved by repetitive treatment with 20% piperidine in DMF. The final product was cleaved from the resin and purified with semipreparative reverse-phase high-performance liquid chromatography (RP-HPLC). The product yield for N_3_S-BN[2-14] was ~40% but <10% for N_3_S-X-BN[2-14]. The chemical purity was >95% for both derivatives. The molecular masses from MS were 1.73 and 2.07 kDa for N_3_S-BN[2-14] and N_3_S-X-BN[2-14], respectively.

Radiolabeling was carried out with radioisotope exchange from the ^99m^Tc^(V)^O gluconate precursor. A solid mixture of sodium gluconate, sodium bicarbonate, and stannous chloride was first dissolved in sodium pertechnetate solution. The solution was then mixed with each BN derivative separately. The mixture (pH 6–7) was allowed to react for 20 min at 37°C, and each radiolabeled BN derivative was purified with RP-HPLC. Both derivatives showed >98% radiochemical yields, and the radiolabeled products remained >90% intact up to 6 h after labeling as determined by analytical RP-HPLC. The RP-HPLC retention time of ^99m^Tc-N_3_S-BN[2-14] was 16.1 min, whereas that of ^99m^Tc-N_3_S-X-BN[2-14] was lower (14.2 min), indicative of the higher hydrophilicity of ^99m^Tc-N_3_S-X-BN[2-14]. The specific activity was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=(99m)Tc-N(3)S-X-Bombesin)]

The metabolic stability of both BN derivatives was studied in human plasma, PC-3 cell culture, as well as kidney and liver homogenates (1). Generally, the catabolic rate of both derivatives was higher in cell culture than in human plasma. During the first 15 min of incubation in human plasma, the percentage of intact ^99m^Tc-N_3_S-BN[2-14] and ^99m^Tc-N_3_S-X-BN[2-14] was ~80% and ~70%, respectively. After 120 min of incubation, both derivatives remained intact at a level of 60%. Degradation of the two derivatives was different in the GRPR-expressing PC-3 cells. After 30 min of incubation with PC-3 cells, ~30% of the ^99m^Tc-N_3_S-BN[2-14] was intact, but ~50% of the ^99m^Tc-N_3_S-X-BN[2-14] was intact. Enzymatic degradation in the kidney and liver homogenates occurred after just 5 min of incubation. In the kidney homogenates, ^99m^Tc-N_3_S-BN[2-14] and ^99m^Tc-N_3_S-X-BN[2-14] remained >40% and >45% parent at 5 min, respectively, and 20–30% intact at 15 min for both. In the liver homogenates, however, ^99m^Tc-N_3_S-BN[2-14] was almost totally degraded within 5 min, whereas >60% of the ^99m^Tc-N_3_S-X-BN[2-14] remained intact. No detectable amount of pertechnetate was released from the breakdown of the chelator ^99m^Tc-Gly-Gly-Cys in all cases.

The binding affinity of the two BN derivatives and of their ^185/187^Re complexes for the GRPR was evaluated in PC-3 cells with a competitive cell binding assay (1). A typical sigmoid curve was obtained for displacement of the GRPR-specific radioligand ^125^I-[Tyr^4^]-BN from PC-3 cells as a function of increasing concentration of the cold ligands. N_3_S-X-BN[2-14] and its ^185/187^Re complex showed better affinity than N_3_S-BN[2-14] and its ^185/187^Re complex. The 50% inhibitory concentration (IC_50_) values were 3.2 ± 0.6 and 3.0 ± 0.7 nmol for N_3_S-BN[2-14] and its ^185/187^Re complex, respectively. The IC_50_ values for N_3_S-X-BN[2-14] and its ^185/187^Re complex were 1.5 ± 0.2 and 2.2 ± 0.1 nmol, respectively.

The internalization and efflux of the BN derivatives were assessed in PC-3 cells at 37°C in the presence (blocking experiments) or absence of native BN (1). After 5 min of incubation, 34% of the ^99m^Tc-N_3_S-BN[2-14] and 66% of the ^99m^Tc-N_3_S-X-BN[2-14] was internalized, reaching 78% and 88% after 120 min, respectively. Measurement of the efflux up to 90 min after 30 min of incubation showed that ~53% of the ^99m^Tc-N_3_S-BN[2-14] and ~63% of the ^99m^Tc-N_3_S-X-BN[2-14] remained trapped in the cells. The detailed data of blocking experiments were not described.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=(99m)Tc-N(3)S-X-Bombesin)]

Biodistribution was first studied in normal Swiss mice (n = 3–5 mice/time point) (1). The two derivatives demonstrated fast, but different, rates of blood clearance. The blood levels (expressed as % injected dose per gram tissue (ID/g)) at 60 min and 120 min after injection were 0.51 ± 0.06 and 0.16 ± 0.06, respectively, for ^99m^Tc-N_3_S-X-BN[2-14], and 1.00 ± 0.17 and 0.46 ± 0.05, respectively, for ^99m^Tc-N_3_S-BN[2-14]. High radioactivity levels were observed in the kidneys, indicating that the predominant excretion for both derivatives was via the kidneys to urine. High uptake was also observed in the GRPR-positive pancreas: 27.89 ± 7.78, 16.72 ± 3.57, and 10.26 ± 1.64% ID/g at 15, 30, and 60 min after injection, respectively, for ^99m^Tc-N_3_S-X-BN[2-14]; 13.38 ± 3.99, 9.49 ± 3.31, and 5.20 ± 3.88% ID/g, respectively, for ^99m^Tc-N_3_S-BN[2-14]. No evident accumulation was observed in the stomach. The liver and intestine also had relatively low uptake, compared with other normal tissues. The uptake levels between the two derivatives at 15, 30, and 60 min were all significantly different in organs of the blood, kidneys, liver, intestines, lungs and pancreas (P < 0.05). Blocking studies showed that uptake in the pancreas was significantly inhibited by co-administration of an excess amount of native BN, being ~63% of the uptake without blocking at 30 min after injection (n = 3 mice/group) (P < 0.05).

Biodistribution was then studied in PC-3 tumor-bearing SCID mice (n = 3 mice/time point) (1). Both ^99m^Tc-N_3_S-BN[2-14] and ^99m^Tc-N_3_S-X-BN[2-14] were capable of rapidly targeting the GRPR-positive pancreas and PC-3 tumor. However, ^99m^Tc-N_3_S-X-BN[2-14] showed a more favorable, statistically different biodistribution than ^99m^Tc-N_3_S-BN[2-14] (P < 0.01). In the tumor and pancreas, the accumulation levels at 30 min after injection were 4.56 ± 0.95 and 11.08 ± 2.76% ID/g, respectively, for ^99m^Tc-N_3_S-BN[2-14], and 5.23 ± 2.10 and 11.07 ± 4.2% ID/g, respectively, for ^99m^Tc-N_3_S-X-BN[2-14]. At 60 min, the levels reduced to 1.02 ± 0.18 and 4.17 ± 0.99% ID/g, respectively, for ^99m^Tc-N_3_S-BN[2-14], but increased to 7.14 ± 0.87 and 27.59 ± 6.86% ID/g, respectively, for ^99m^Tc-N_3_S-X-BN[2-14]. At this time point, the tumor/nontarget ratios for ^99m^Tc-N_3_S-X-BN[2-14] were significantly higher than those for ^99m^Tc-N_3_S-BN[2-14] as to the blood (6.67 versus 1.96), muscles (14 versus 9.27), liver (2.9 versus 0.66), and kidneys (0.28 versus 0.18) (P < 0.05). The radioactivity level of ^99m^Tc-N_3_S-X-BN[2-14] in the tumor remained high at 120 min (7.92 ± 0.79% ID/g), with even higher tumor/nontarget ratios than that at 60 min (P < 0.05), showing 33.32 to the blood, 15.53 to the muscles, 3.02 to the liver, and 0.49 to the kidneys. For the blood clearance, both derivatives were cleared efficiently within 60 min, with blood levels of 0.52 ± 0.05 and 1.07 ± 0.12% ID/g for ^99m^Tc-N_3_S-BN[2-14] and ^99m^Tc-N_3_S-X-BN[2-14], respectively. The kidney had the highest radioactivity levels of both derivatives among the organs examined, indicating that they were mainly excreted via the kidneys. At 60 min, the radioactivity level in the kidneys was 5.56 ± 0.52% ID/g for ^99m^Tc-N_3_S-BN[2-14] and 25.49 ± 1.61% ID/g for ^99m^Tc-N_3_S-X-BN[2-14]. The intestinal uptake reached the maximum at 30 min for ^99m^Tc-N_3_S-BN[2-14] (2.08 ± 1.55% ID/g) and at 120 min for ^99m^Tc-N_3_S-X-BN[2-14] (6.75 ± 0.91% ID/g). The liver accumulation was relatively low at all time points for both derivatives.

Blocking studies in PC-3 tumor-bearing SCID mice (n = 3 mice) showed that uptake of ^99m^Tc-N_3_S-BN[2-14] in the pancreas and tumor was significantly inhibited with co-administration of an excess amount of native BN, being 1.69 ± 1.42% ID/g (~85% decrease) and 0.91 ± 0.60% ID/g (~80% decrease), respectively, at 30 min after co-injection (P < 0.05). The blocking studies were not shown for ^99m^Tc-N_3_S-X-BN[2-14].

Dynamic in vivo imaging demonstrated that PC-3 tumors were visible with clear contrast from the adjacent background as early as 10 min after injection and remained observable up to 120 min (1). Prominent uptake was also observed in the kidneys. Administration of a high dose of native BN along with the ^99m^Tc-N_3_S-X-BN[2-14] led to undetectable tumor.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Fragogeorgi E.A., Zikos C., Gourni E., Bouziotis P., Paravatou-Petsotas M., Loudos G., Mitsokapas N., Xanthopoulos S., Mavri-Vavayanni M., Livaniou E., Varvarigou A.D., Archimandritis S.C. (2009). Spacer Site Modifications for the Improvement of the in Vitro and in Vivo Binding Properties of (99m)Tc-N(3)S-X-Bombesin[2-14] Derivatives. Bioconjug Chem.
2 Maina T., Nock B.A., Zhang H., Nikolopoulou A., Waser B., Reubi J.C., Maecke H.R. (2005). Species differences of bombesin analog interactions with GRP-R define the choice of animal models in the development of GRP-R-targeting drugs. J Nucl Med.
3 Smith C.J., Volkert W.A., Hoffman T.J. (2003). Gastrin releasing peptide (GRP) receptor targeted radiopharmaceuticals: a concise update. Nucl Med Biol.
4 Erspamer V., Erpamer G.F., Inselvini M. (1970). Some pharmacological actions of alytesin and bombesin. J Pharm Pharmacol.
5 Smith C.J., Volkert W.A., Hoffman T.J. (2005). Radiolabeled peptide conjugates for targeting of the bombesin receptor superfamily subtypes. Nucl Med Biol.
6 Ananias H.J., de Jong I.J., Dierckx R.A., van de Wiele C., Helfrich W., Elsinga P.H. (2008). Nuclear imaging of prostate cancer with gastrin-releasing-peptide-receptor targeted radiopharmaceuticals. Curr Pharm Des.
7 Ischia J., Patel O., Shulkes A., Baldwin G.S. (2009). Gastrin-releasing peptide: different forms, different functions. Biofactors.
8 Maina T., Nock B., Mather S. (2006). Targeting prostate cancer with radiolabelled bombesins. Cancer Imaging.
9 Weber H.C. (2009). Regulation and signaling of human bombesin receptors and their biological effects. Curr Opin Endocrinol Diabetes Obes.
10 Yang Y.S., Zhang X., Xiong Z., Chen X. (2006). Comparative in vitro and in vivo evaluation of two 64Cu-labeled bombesin analogs in a mouse model of human prostate adenocarcinoma. Nucl Med Biol.
11 Liu S., Edwards D.S., Barrett J.A. (1997). 99mTc labeling of highly potent small peptides. Bioconjug Chem.
12 Zhang X., Cai W., Cao F., Schreibmann E., Wu Y., Wu J.C., Xing L., Chen X. (2006). 18F-labeled bombesin analogs for targeting GRP receptor-expressing prostate cancer. J Nucl Med.
13 Schroeder R.P., van Weerden W.M., Bangma C., Krenning E.P., de Jong M. (2009). Peptide receptor imaging of prostate cancer with radiolabelled bombesin analogues. Methods.
14 Chen X., Park R., Hou Y., Tohme M., Shahinian A.H., Bading J.R., Conti P.S. (2004). microPET and autoradiographic imaging of GRP receptor expression with 64Cu-DOTA-[Lys3]bombesin in human prostate adenocarcinoma xenografts. J Nucl Med.
15 Hohne A., Mu L., Honer M., Schubiger P.A., Ametamey S.M., Graham K., Stellfeld T., Borkowski S., Berndorff D., Klar U., Voigtmann U., Cyr J.E., Friebe M., Dinkelborg L., Srinivasan A. (2008). Synthesis, 18F-labeling, and in vitro and in vivo studies of bombesin peptides modified with silicon-based building blocks. Bioconjug Chem.
16 Li Z.B., Wu Z., Chen K., Ryu E.K., Chen X. (2008). 18F-labeled BBN-RGD heterodimer for prostate cancer imaging. J Nucl Med.
17 Prasanphanich A.F., Retzloff L., Lane S.R., Nanda P.K., Sieckman G.L., Rold T.L., Ma L., Figueroa S.D., Sublett S.V., Hoffman T.J., Smith C.J. (2009). In vitro and in vivo analysis of [(64)Cu-NO2A-8-Aoc-BBN(7-14)NH(2)]: a site-directed radiopharmaceutical for positron-emission tomography imaging of T-47D human breast cancer tumors. Nucl Med Biol.
18 Santos-Cuevas C.L., Ferro-Flores G., Arteaga de Murphy C., Ramirez Fde M., Luna-Gutierrez M.A., Pedraza-Lopez M., Garcia-Becerra R., Ordaz-Rosado D. (2009). Design, preparation, in vitro and in vivo evaluation of (99m)Tc-N2S2-Tat(49-57)-bombesin: a target-specific hybrid radiopharmaceutical. Int J Pharm.
19 Nock B., Nikolopoulou A., Chiotellis E., Loudos G., Maintas D., Reubi J.C., Maina T. (2003). [99mTc]Demobesin 1, a novel potent bombesin analogue for GRP receptor-targeted tumour imaging. Eur J Nucl Med Mol Imaging.
20 Cescato R., Maina T., Nock B., Nikolopoulou A., Charalambidis D., Piccand V., Reubi J.C. (2008). Bombesin receptor antagonists may be preferable to agonists for tumor targeting. J Nucl Med.
21 Nock B.A., Nikolopoulou A., Galanis A., Cordopatis P., Waser B., Reubi J.C., Maina T. (2005). Potent bombesin-like peptides for GRP-receptor targeting of tumors with 99mTc: a preclinical study. J Med Chem.